# ^99m^Tc-Diethylenetriamine pentaacetic acid superparamagnetic iron oxide nanoparticles conjugated with lactobionic acid

Chemical name: | ^99m^Tc-Diethylenetriamine pentaacetic acid superparamagnetic iron oxide nanoparticles conjugated with lactobionic acid
Abbreviated name: | ^99m^Tc-DTPA-SPION-LBA
Synonym:
Agent category: | Compound
Target: | Asialoglycoprotein receptors (ASGP-Rs)
Target category: | Receptor
Method of detection: | Magnetic resonance imaging (MRI), single-photon emission computed tomography (SPECT)
Source of signal: | Iron oxide, ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4502251), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/186910312) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=432) for more information about ASGP-R.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SPION%20Asialoglycoprotein)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used in imaging because of their abundance in water molecules. Water comprises ~80% of most soft tissue. The contrast of proton MRI depends primarily on the density of the nuclear proton spins, the relaxation times of the nuclear magnetization (T1, longitudinal, and T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the development of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide (CLIO) nanoparticles and other iron oxide formulations affect T2 primarily and lead to decreased signals. On the other hand, paramagnetic T1 agents, such as gadolinium (Gd^3+^) and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images.

The superparamagnetic iron oxide (SPIO) structure is composed of ferric iron (Fe^3+^) and ferrous iron (Fe^2+^). The iron oxide particles are coated with a protective layer of dextran or other polysaccharide. These particles have large combined magnetic moments or spins, which are randomly rotated in the absence of an applied magnetic field. SPIO is used mainly as a T2 contrast agent in MRI, though it can shorten both T1 and T2/T2* relaxation processes. SPIO particle uptake into the reticuloendothelial system occurs by endocytosis or phagocytosis. SPIO particles are also taken up by phagocytic cells such as monocytes, macrophages, and oligodendroglial cells. A variety of cells can also be labeled with these particles for cell trafficking and tumor-specific imaging studies. SPIO agents are classified by their sizes with coating material (~20–3,500 nm in diameter) as large SPIO (LSPIO) nanoparticles, standard SPIO (SSPIO) nanoparticles, ultrasmall SPIO (USPIO) nanoparticles, and monocrystalline iron oxide nanoparticles (MION) (1).

Asialoglycoprotein (ASGP) is specifically taken into mammalian hepatocytes by binding to ASGP receptors (ASGP-Rs) (2). The galactosyl moiety of ASGP is recognized on the surface of hepatocytes and is bound by ASGP-R. The ASGP–ASGP-R complex on the cell surface is subsequently taken into cytoplasm by endocytosis and transferred to lysosomes. ASGP-R is then dissociated from ASGP and recycled to the cell surface. ASGP is degraded in the lysosomes and excreted into the bile. The number of ASGP-Rs on the hepatocytes of individuals with liver disease decreases and is thus considered a good indicator for the evaluation of liver function. Because ASGP-R recognizes galactose, ^99m^Tc-diethylenetriamine pentaacetic acid-galactosyl-human serum albumin (^99m^Tc-GSA) (3, 4) and ^99m^Tc-galactosyl-neoglycoalbumin (^99m^Tc-NGA) (5) are ASGP-R probes that accumulate specifically in the liver and are used for liver scintigraphy to determine liver mass and function. SPIO nanoparticles (SPION) modified with dopamine were conjugated with lactobionic acid (LBA) and diethylenetriamine pentaacetic acid (DTPA) to form DTPA-SPION-LBA (6). Each LBA contains one galactosyl moiety for binding to ASGP-Rs. DTPA-SPION-LBA were labeled with ^99m^Tc as a multimodality (single-photon emission computed tomography (SPECT) and MR) imaging agent of ASGP-Rs in the liver.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=ASGP-R%5BAll+Fields%5D+AND+micad%5Bbook%5D)
- Gene information in NCBI (ASGP-Rs (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=ASGP-r%5BAll+Fields%5D+AND+(%22Homo+sapiens%22%5BOrganism%5D+OR+(%22Homo+sapiens%22%5BOrganism%5D+OR+human%5BAll+Fields%5D)))).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=Asialoglycoprotein)
- Clinical trials (ASGP-Rs (http://www.clinicaltrials.gov/ct2/results?term=Asialoglycoprotein))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SPION%20Asialoglycoprotein%20and%20synthesis)]

SPION (12 nm) were coated with dopamine using the method of Shultz et al. (7). In brief, SPION (10 mg in 5 ml toluene) were mixed with 50 mg dopamine for 30 min in a sonication bath. A solution of 1-ethyl-3-(3-(dimethylamino)-propyl)carbodiimide and N-hydroxysuccinimide was added to a solution of dopamine-coated SPION and LBA (6). The mixture was incubated for 48 h at room temperature. SPION-LBA were isolated magnetically and centrifuged to remove larger particles. Subsequently, DTPA was conjugated to the free amine group of dopamine on the surface of SPION with 2-(4-isothiocyanatobenzyl)-DTPA. There were ~2 DTPA molecules per SPION. A mixture of DTPA-SPION-LBA (0.5 mg), SbCl_2_ (0.002 mg), and ^99m^Tc (46.3 MBq (1.25 mCi)) was incubated for 30 min at room temperature. The radiolabeling yield was >95%. The number of LBA molecules per SPION was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SPION%20Asialoglycoprotein%20and%20in%20vitro)]

Lee et al. (6) performed in vitro uptake studies of DTPA-SPION-LBA (100 µg/ml) and SPION (100 µg/ml) in cultured human hepatoblastoma HepG2 cells, which were shown to express ASPG-Rs. A strong uptake of DTPA-SPION-LBA was observed at 2 h after incubation as measured with Prussian blue staining of Fe in the cytoplasm of the cells, whereas there was little accumulation of SPION.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SPION%20Asialoglycoprotein%20and%20rodentia)]

Lee et al. (6) performed ex vivo biodistribution studies of ^99m^Tc-DTPA-SPION-LBA in normal mice (n = 4) at 1 h after injection. The radioactivity levels in percent injected dose per gram (% ID/g) were 38.43, 18.69, 12.22, 11.48, 4.88, and 1.30 for the liver, spleen, lung, kidney, blood, and intestine, respectively. SPECT/CT imaging showed that the liver, urinary bladder, and lung were clearly visualized at 1 h after injection. The liver/muscle ratio was 24.1. Coinjection of 0.085 and 0.115 mmol galactose with ^99m^Tc-DTPA-SPION-LBA reduced the liver/muscle ratio to 14.9 and 7.2, respectively. MRI of the liver showed a 51% reduction (n = 3) of T2 signal (1.5 T) at 1 h after SPION-LBA injection. Transmission electron microscopy of liver section showed the presence of 30-nm nanoparticles containing ~12-nm, electron-dense particles in the cytoplasm and mitochondrial matrix.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SPION%20Asialoglycoprotein%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SPION%20Asialoglycoprotein%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SPION%20Asialoglycoprotein%20and%20human)]

No publication is currently available.

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Stockert R.J. (1995). The asialoglycoprotein receptor: relationships between structure, function, and expression. Physiol Rev.
3 Kwon A.H., Ha-Kawa S.K., Uetsuji S., Kamiyama Y., Tanaka Y. (1995). Use of technetium 99m diethylenetriamine-pentaacetic acid-galactosyl-human serum albumin liver scintigraphy in the evaluation of preoperative and postoperative hepatic functional reserve for hepatectomy. Surgery.
4 Wu J., Ishikawa N., Takeda T., Tanaka Y., Pan X.Q., Sato M., Todoroki T., Hatakeyama R., Itai Y. (1995). The functional hepatic volume assessed by 99mTc-GSA hepatic scintigraphy. Ann Nucl Med.
5 Vera D.R., Stadalnik R.C., Krohn K.A. (1985). Technetium-99m galactosyl-neoglycoalbumin: preparation and preclinical studies. J Nucl Med.
6 Lee C.M., Jeong H.J., Kim E.M., Kim D.W., Lim S.T., Kim H.T., Park I.K., Jeong Y.Y., Kim J.W., Sohn M.H. (2009). Superparamagnetic iron oxide nanoparticles as a dual imaging probe for targeting hepatocytes in vivo. Magn Reson Med.
7 Shultz M.D., Reveles J.U., Khanna S.N., Carpenter E.E. (2007). Reactive nature of dopamine as a surface functionalization agent in iron oxide nanoparticles. J Am Chem Soc.